# Ferumoxtran

Chemical name: | Ferumoxtran
Abbreviated name: | USPIO
Synonym: | Ultrasmall Superparamagnetic Iron Oxide, AMI-227, NC100150
Agent Category: | Superparamagnetic Iron Oxide
Target: | Reticuloendothelial system
Target Category: | Internalized by phagocytes
Method of detection: | Magnetic Resonance imaging (MRI)
Source of signal\contrast: | Iron oxide
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals; - Non-human primates; - Humans | No structure is available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22ferumoxtran%22%5BSubstance%20Name%5D)]

Magnetic resonance imaging (MRI) maps information about tissues spatially and functionally. Protons (hydrogen nuclei) are widely used to create images because of their abundance in water molecules. Water comprises about 80% of most soft tissues. The contrast of proton MRI depends mainly on the density of nuclear (proton spins), the relaxation times of the nuclear magnetization (T1, longitudinal and T2, transverse), the magnetic environment of the tissues, and the blood flow to the tissues. However, insufficient contrast between normal and diseased tissues requires development of contrast agents. Most of the contrast agents affect the T1 and T2 relaxation of the surrounding nuclei, mainly the protons of water. T-2* is the spin-spin relaxation time composed of variations from molecular interactions and intrinsic magnetic heterogeneities of tissues in the magnetic field (1).

Superparamagnetic iron oxide (SPIO) structure is composed of ferric iron (Fe^3+^) and ferrous iron (Fe^2+^). The iron oxides particles are coated with a layer of dextran or other polysaccharide. These particles have a large combined magnetic moments or spins which are randomly rotated in the absence of an applied magnetic field. SPIO is used mainly as a T2 contrast agent in MRI though it can shorten both T1 and T2/T2* relaxation processes. SPIO particle uptake into reticuloendothelial system (RES) is by endocytosis or phagocytosis. SPIO particles are taken up by phagocytic cells such as monocytes, macrophages, and oligodendroglial cells. A variety of cells can also be labeled with these particles for cell trafficking and tumor-specific imaging studies. SPIO agents are classified by their sizes with coating material (about 20 nm to 3,500 nm in diameters) as large SPIO agents (Ferumoxsil or AMI-121, Ferucarbotran, OMP), standard SPIO (SSPIO) agents (Ferumoxides or AMI-25, SHU 555), ultrasmall SPIO (USPIO) agents (Ferumoxtran or AMI-227, NC100150) and monocrystalline iron oxide nanoparticles (MION) agents (1).

Ferumoxtran is composed of iron particles of about 4-6 nm and the hydrodynamic diameter is about 20-40 nm. The crystals are covered with a layer of dextran. Ferumoxtran is classified as USPIO with significant T1 relaxation effects. Ferumoxtran has a long plasma half-life due to improved coating. In humans, the blood pool half-life of plasma relaxation times is calculated to be more than 24 h (2). Because of its long blood half-life, ferumoxtran can be used as blood pool agent during the early phase of intravenous administration (3). In the late phase, ferumoxtran is suitable for the evaluation of RES in the body, particularly in lymph nodes (4).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22ferumoxtran%22%5BSubstance%20Name%5D%20AND%20synthesis)]

SPIO agents are produced by controlling the precipitation of iron oxide in an aqueous solution of ferric salt, ferrous salt, and coating material by addition of an alkaline solution while active stirring or sonication is applied. The desired SPIO size of the agent is isolated and purified by differential column chromatography, centrifugation, and dialysis. Electron microscopy, X-ray diffraction and laser light scattering are used to measure median diameter of the nanoparticles. Relaxivities are measured by NMR spectroscopy (1).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22ferumoxtran%22%5BSubstance%20Name%5D%20AND%20in%20vitro)]

It was shown that the uptake of SPIO by human monocytes was dependent on size, concentration, and time. SSPIO uptake was higher than USPIO (AMI-227) uptake as measured by iron content and T2* relaxivity. The uptakes of both were directly proportional to concentration and time. The surface property of SPIO is also an important factor. MION was also taken up by T-cells, glioma cells and macrophages. MION can be attached to monoclonal and polyclonal antibodies for cell-surface markers of tumor cells and inflammatory cells accessible via blood circulation (5) (6).

Using monolayers of cultured pig endothelial cells to measure transcytosis of particles, 45% of USPIO nanoparticles were translocated in 5.5 h, whereas only 11% of SSPIO nanoparticles were translocated (7). On a human activated monocyte THP-1 cell assay, SSPIO showed a higher macrophage uptake (1.1-3.0%) compared with USPIO, ferumoxtran (0.03-0.12%) (6). These differences are attributed to the larger size of SSPIO nanoparticles.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22ferumoxtran%22%5BSubstance%20Name%5D%20AND%20rodentia)]

The blood half-life of ferumoxtran (the hydrodynamic diameter is about 11 nm) in rats was 81 min, considerably longer than that of larger SPIO preparations, such as AMI-25 (6 min). Electron microscopy demonstrated that ferumoxtran particles transmigrate the capillary wall by means of vesicular transport and through interendothelial junctions. Twenty-four h after intravenous administration, 3.6% of the injected dose/gram (ID/g) of tissue was found in lymph nodes, 2.9% ID/g in bone marrow, 6.3% ID/g in liver, and 7.1% ID/g in spleen (7). In another study, ferumoxtran was found to be mainly as an extracellular agent for at least 1 h in the rats (0.15 mmol Fe/kg). Liver RES accumulation peaked at 8-24 hours. There was no substantial uptake within hepatocytes (8).

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22ferumoxtran%22%5BSubstance%20Name%5D%20AND%20primates%20not%20humans)]

Bourrinet et al. (9) performed pharmacokinetic, safety pharmacology, single- and repeat-dose toxicity, reproduction toxicity, and genotoxicity studies with ferumoxtran-10 given intravenously in mice, rats, rabbits, dogs, and monkeys. Ferumoxtran-10 was taken up by macrophages in liver, spleen, and lymph nodes within 24 hours after injection and underwent progressive metabolism. The blood clearance pattern in monkeys exhibited a two-phase model with a half-life (t_1/2_α) of 52 min during the distribution phase and a half-life (t_1/2_ß) of 342 min during the elimination phase. Toxicity was observed only at very high exposure levels, well above the intended human dose of 2.6 mg Fe/kg.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22ferumoxtran%22%5BSubstance%20Name%5D%20AND%20%28dog%20or%20pig%20or%20rabbit%20or%20sheep%29)]

Ferumoxtran contrast agents have been studied in renal perfusion, portal angiography, cardiac ischemia, inflammation, and atherosclerosis using dogs [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22ferumoxtran%22%5BSubstance%20Name%5D%20AND%20%28%22dogs%22%5BMeSH%20Terms%5D%20OR%20dogs%5BText%20Word%5D%29)], pigs [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22ferumoxtran%22%5BSubstance%20Name%5D%20AND%20%28%22swine%22%5BMeSH%20Terms%5D%20OR%20pigs%5BText%20Word%5D%29)], and rabbits [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22ferumoxtran%22%5BSubstance%20Name%5D%20AND%20%28%22rabbits%22%5BMeSH%20Terms%5D%20OR%20rabbit%5BText%20Word%5D%29)].

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22ferumoxtran%22%5BSubstance%20Name%5D%20AND%20humans)]

AMI-227 was studied in 41 healthy subjects. Relaxation time measurements in plasma samples showed a strong, dose-dependent, and persistent decrease in T1 and T2 values. Significant changes in MR signal intensity of the blood pool and well-perfused organs (liver and spleen) were noted on both T1- and T2- weighted images. Changes in signal intensity of cervical lymph nodes were also observed at the higher doses and late imaging times (2). The major potential applications for USPIO nanoparticles are as (a) an intravenous contrast agent for the lymph nodes [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22ferumoxtran%22%5BSubstance%20Name%5D%20AND%20%22humans%22%5BMeSH%20Terms%5D%20AND%20%22lymph%20nodes%22%5BMeSH%5D)], (b) a bone marrow contrast agent (10), [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22ferumoxtran%22%5BSubstance%20Name%5D%20AND%20%22humans%22%5BMeSH%20Terms%5D%20AND%20%28%22bone%20marrow%22%5BMeSH%20Terms%5D%20OR%20bone%20marrow%5BText%20Word%5D%29)], (c) a perfusion agent for angiography [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22ferumoxtran%22%5BSubstance%20Name%5D%20AND%20%22humans%22%5BMeSH%20Terms%5D%20AND%20%22angiography%22%5BMeSH%20Terms%5D)], (d) a perfusion agent for the brain and kidneys [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22ferumoxtran%22%5BSubstance%20Name%5D%20AND%20%22humans%22%5BMeSH%20Terms%5D%20AND%20%28%22brain%22%5BMeSH%20Terms%5D%20OR%20%22kidney%22%5BMeSH%20Terms%5D%29)], and (e) a monitoring agent for macrophage infiltration in pathological tissues [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22ferumoxtran%22%5BSubstance%20Name%5D%20AND%20%22humans%22%5BMeSH%5D%20AND%20%22arteriosclerosis%22%5BMeSH%5D)].

## References

1 Wang Y.X., Hussain S.M., Krestin G.P. (2001). Superparamagnetic iron oxide contrast agents: physicochemical characteristics and applications in MR imaging. Eur Radiol.
2 McLachlan S.J., Morris M.R., Lucas M.A., Fisco R.A., Eakins M.N., Fowler D.R., Scheetz R.B., Olukotun A.Y. (1994). Phase I clinical evaluation of a new iron oxide MR contrast agent. J Magn Reson Imaging.
3 Stillman A.E., Wilke N., Li D., Haacke M., McLachlan S. (1996). Ultrasmall superparamagnetic iron oxide to enhance MRA of the renal and coronary arteries: studies in human patients. J Comput Assist Tomogr.
4 Anzai Y., Piccoli C.W., Outwater E.K., Stanford W., Bluemke D.A., Nurenberg P., Saini S., Maravilla K.R., Feldman D.E., Schmiedl U.P., Brunberg J.A., Francis I.R., Harms S.E., Som P.M., Tempany C.M. (2003). Evaluation of neck and body metastases to nodes with ferumoxtran 10-enhanced MR imaging: phase III safety and efficacy study. Radiology.
5 Metz S., Bonaterra G., Rudelius M., Settles M., Rummeny E.J., Daldrup-Link H.E. (2004). Capacity of human monocytes to phagocytose approved iron oxide MR contrast agents in vitro. Eur Radiol.
6 Raynal I., Prigent P., Peyramaure S., Najid A., Rebuzzi C., Corot C. (2004). Macrophage endocytosis of superparamagnetic iron oxide nanoparticles: mechanisms and comparison of ferumoxides and ferumoxtran-10. Invest Radiol.
7 Weissleder R., Elizondo G., Wittenberg J., Rabito C.A., Bengele H.H., Josephson L. (1990). Ultrasmall superparamagnetic iron oxide: characterization of a new class of contrast agents for MR imaging. Radiology.
8 Van Beers B.E., Sempoux C., Materne R., Delos M., Smith A.M. (2001). Biodistribution of ultrasmall iron oxide particles in the rat liver. J Magn Reson Imaging.
9 Bourrinet P., Bengele H.H., Bonnemain B., Dencausse A., Idee J.M., Jacobs P.M., Lewis J.M. (2006). Preclinical safety and pharmacokinetic profile of ferumoxtran-10, an ultrasmall superparamagnetic iron oxide magnetic resonance contrast agent. Invest Radiol.
10 Daldrup-Link H.E., Rummeny E.J., Ihssen B., Kienast J., Link T.M. (2002). Iron-oxide-enhanced MR imaging of bone marrow in patients with non-Hodgkin's lymphoma: differentiation between tumor infiltration and hypercellular bone marrow. Eur Radiol.